# ^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-His

Chemical name: | ^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-His
Abbreviated name: | ^99m^Tc-L19-His
Synonym: | ^99m^Tc-scFv L19-His, ^99m^Tc-anti-ED-B FN scFv Ab
Agent Category: | Single-chain Antibody fragment (scFv)
Target: | ED-B Fibronectin (ED-B FN)
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about ED-B fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29)]

^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-His (^99m^Tc-L19-His) is a radiolabeled molecular imaging agent developed for single-photon emission computed tomography (SPECT) imaging of tumor angiogenesis and guidance for antiangiogenic treatment (1). ^99m^Tc is a gamma emitter with a half-life (t_½_) of 6.01 h.

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels (2). Tumor growth depends on the formation of new blood vessels from this process. Normal angiogenesis is orderly and highly regulated, whereas tumor angiogenesis is chaotic and irregular. Abnormal angiogenesis is important in the carcinogenesis, growth, and progression of solid and hematologic tumors in humans (3). Fibronectins (FNs) are a family of universal cell-adhesion molecules that are widely distributed (1). FN is a polymorphic glycoprotein of ~2500 amino acids and has a high molecular mass of 250–280 kDa. FN occurs in soluble form in plasma and other body fluids and in insoluble form in the extracellular matrices (4, 5). Both forms are dimers composed of a series of repeating units of three types and joined by two disulfide bonds at the C-terminus of the molecule. FN polymorphism arises from alternative splicing patterns of the pre-mRNA or post-translational modifications of FN itself (5). Alternative splicing in three regions [extra domain A (ED-A), extra domain B (ED-B), and type III homology connecting segment (IIICS)] may generate 20 different FN subunit isoforms. The splice variant ED-B FN, which is highly expressed during angiogenesis in both neoplastic and normal tissues (6), is an oncofetal antigen expressed at different levels in the stroma associated with the neovasculature of solid tumors. High levels of ED-B expression have been found in primary and metastatic tumors in breast, colorectal, and non-small cell lung cancers (1, 7-9).

Molecular imaging of angiogenesis offers serial non-invasive evaluation of both location and growth dynamics of tumors (10). SPECT or positron emission tomography imaging with an appropriate radiolabeled tracer targeted to angiogenic pathways may allow the evaluation of specific aspects of tumor vascular biology (9). A molecular probe that targets ED-B FN can be both an early tumor marker and a tool to monitor the success of antiangiogenic cancer therapy. The single-chain antibody fragment (scFv) L19, which has a high affinity for ED-B FN, was developed by Pini et al. (11). Radioiodinated L19 showed specific accumulation around tumor neovasculature and tumor stroma with high ED-B expression (12, 13). In an effort to prepare a stable ^99m^Tc-labeled L19, Berndorff et al. (1) genetically introduced a (His)_6_ peptide sequence at the C-terminus of L19 to produce L19-His molecules. Two other L19 derivatives, AP39 and L19-Hi20, were also prepared for radiolabeling. These ^99m^Tc-labeled L19 derivatives appeared to have favorable biodistribution and imaging properties in mice bearing murine embryonal teratocarcinomas (F9). However, the study did not provide data to confirm that the binding was a result of angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20synthesis)]

Pini et al. (11) constructed and used a large synthetic phage display human antibody library (>3 × 10^8^ clones) to produce L19 with a very high affinity (dissociation constant (K_d_) = 54 pM) for the ED-B domain of FN. L19 was cloned in scFv configuration in the novel phagemid vector pDN332. Berndorff et al. (1) prepared the L19 derivative by modifying the sequence of scFv LP19 to encode the (His)_6_ domain at the C-terminal end of the V_L_ chain. The DNA sequence encoding this LP19 derivative was cloned into the prokaryotic expression vector pDN5 with isopropyl-1-thio-β-D-galactoside–inducible promoter and ampicillin resistance marker. L19-His was purified by affinity chromatography before radiolabeling. Radiolabeling was performed according to the tricarbonyl method (1, 14, 15). In this method, L19-His was labeled with ^99m^Tc by the formation of the precursor [^99m^Tc(OH_2_)_3_(CO)_3_]^+^. [^99m^Tc(OH_2_)_3_(CO)_3_]^+^ was prepared via one-pot synthesis with potassium boranocarbonate and ^99m^Tc-pertechnetate (16), and it was purified by high-performance liquid chromatography (HPLC). Approximately 100 μg of L19-His in 10 mmol/L N-(2-hydroxyethyl)piperazine-N'-(2-ethanesulfonic acid) buffer (pH 7.5) was added to 37 MBq (1 mCi) [^99m^Tc(OH_2_)_3_(CO)_3_]^+^ solution. The mixture was incubated for 1 h at 37ºC. ^99m^Tc-L19-His was purified by affinity chromatography. HPLC analysis showed that ^99m^Tc- L19-His was a dimer. The radiochemical yield was >93%, and the specific activity was 9 MBq/nmol (dimer; 0.24 mCi/nmol). No yield was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20in%20vitro)]

Berndorff et al. (1) determined the in vitro immunoreactivity of ^99m^Tc-L19-His by using affinity chromatography with ED-B FN–conjugated Sepharose. ^99m^Tc-L19-His showed an immunoreactivity of 89%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20rodentia)]

Biodistribution studies (n = 3) of ^99m^Tc-L19-His were performed in nude mice bearing murine F9 tumors (1). F9 tumors were previously reported to express high levels of ED-B FN (13). ^99m^Tc-AP39 showed rapid blood clearance and radioactivity localization in the tumor. The radioactivity levels of ^99m^Tc-L19-His (percentage of injected dose per g (% ID/g)) in the tumors were 6.3 ± 2.0 (0.25 h), 8.4 ± 0.9 (1 h), 9.4 ± 1.4 (3 h), 8.1 ± 2.0 (5 h), and 5.7 ± 2.0 (24 h). The tumor/blood ratios were 0.4 ± 0.1 (0.25 h), 2.0 ± 0.2 (1 h), 5.7 ± 0.5 (3 h), 9.5 ± 2.6 (5 h), and 23.6 ± 8.3 (24 h). ^99m^Tc-L19-His appeared to be excreted primarily by the kidneys, radioactivity levels in the kidneys were 87.2 ± 4.2% ID/g and 72.4 ± 11.3% ID/g at 0.25 and 24 h, respectively. Only ~32.4% ID was excreted via the urine after 24 h. ^99m^Tc-L19-His radioactivity also accumulated in the ED-B FN-expression reproductive organs (ovaries, and uterus). At 0.25 h, the radioactivity levels (% ID/g) in other major organs were 27.2 ± 18.8 (ovaries), 18.7 ± 2.0 (blood), 10.4 ± 1.8 (lungs), 6.1 ± 0.7 (liver), 5.5 ± 0.6 (spleen), 4.9 ± 1.5 (thyroid), 3.2 ± 1.7 (uterus), and 2.0 ± 0.2 (stomach). By 24 h, these radioactivity levels (% ID/g) decreased to 2.8 ± 0.5 (ovaries), 5.7 ± 2.0 (blood), 2.0 ± 0.6 (lungs), 2.5 ± 0.7 (liver), 0.8 ± 0.2 (spleen), 4.4 ± 2.4 (uterus), 1.1 ± 0.0 (thyroid), and 1.1 ± 0.2 (stomach). No specific blocking study was performed.

Gamma imaging was performed in mice bearing s.c. F9 tumors (80–100 mm^2^) (1). Each mouse was injected with 4–7 MBq (0.11–0.19 mCi) ^99m^Tc-L19-His. Imaging with ^99m^Tc-L19-His produced clear tumor images at 5 and 24 h. The background was low except for high radioactivity accumulation in the kidneys. The kidneys were visualized even at 24 h. The liver was slightly detectable after 5 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-His%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20human)]

No publication is currently available.

## References

1 Berndorff D., Borkowski S., Moosmayer D., Viti F., Muller-Tiemann B., Sieger S., Friebe M., Hilger C.S., Zardi L., Neri D., Dinkelborg L.M. (2006). Imaging of tumor angiogenesis using 99mTc-labeled human recombinant anti-ED-B fibronectin antibody fragments. J Nucl Med.
2 Shinkaruk S., Bayle M., Lain G., Deleris G. (2003). Vascular endothelial cell growth factor (VEGF), an emerging target for cancer chemotherapy. Curr Med Chem Anticancer Agents.
3 Ranieri G., Patruno R., Ruggieri E., Montemurro S., Valerio P., Ribatti D. (2006). Vascular endothelial growth factor (VEGF) as a target of bevacizumab in cancer: from the biology to the clinic. Curr Med Chem.
4 Carnemolla B., Balza E., Siri A., Zardi L., Nicotra M.R., Bigotti A., Natali P.G. (1989). A tumor-associated fibronectin isoform generated by alternative splicing of messenger RNA precursors. J Cell Biol.
5 Kosmehl H., Berndt A., Katenkamp D. (1996). Molecular variants of fibronectin and laminin: structure, physiological occurrence and histopathological aspects. Virchows Arch.
6 Castellani P., Viale G., Dorcaratto A., Nicolo G., Kaczmarek J., Querze G., Zardi L. (1994). The fibronectin isoform containing the ED-B oncofetal domain: a marker of angiogenesis. Int J Cancer.
7 Kaczmarek J., Castellani P., Nicolo G., Spina B., Allemanni G., Zardi L. (1994). Distribution of oncofetal fibronectin isoforms in normal, hyperplastic and neoplastic human breast tissues. Int J Cancer.
8 Pujuguet P., Hammann A., Moutet M., Samuel J.L., Martin F., Martin M. (1996). Expression of fibronectin ED-A+ and ED-B+ isoforms by human and experimental colorectal cancer. Contribution of cancer cells and tumor-associated myofibroblasts. Am J Pathol.
9 Santimaria M., Moscatelli G., Viale G.L., Giovannoni L., Neri G., Viti F., Leprini A., Borsi L., Castellani P., Zardi L., Neri D., Riva P. (2003). Immunoscintigraphic detection of the ED-B domain of fibronectin, a marker of angiogenesis, in patients with cancer. Clin Cancer Res.
10. Laking, G.R. and P.M. Price, Positron emission tomographic imaging of angiogenesis and vascular function. Br J Radiol, 2003. 76 Spec No 1: p. S50-9.
11 Pini A., Viti F., Santucci A., Carnemolla B., Zardi L., Neri P., Neri D. (1998). Design and use of a phage display library. Human antibodies with subnanomolar affinity against a marker of angiogenesis eluted from a two-dimensional gel. J Biol Chem.
12 Tarli L., Balza E., Viti F., Borsi L., Castellani P., Berndorff D., Dinkelborg L., Neri D., Zardi L. (1999). A high-affinity human antibody that targets tumoral blood vessels. Blood.
13 Borsi L., Balza E., Bestagno M., Castellani P., Carnemolla B., Biro A., Leprini A., Sepulveda J., Burrone O., Neri D., Zardi L. (2002). Selective targeting of tumoral vasculature: comparison of different formats of an antibody (L19) to the ED-B domain of fibronectin. Int J Cancer.
14 Stalteri M.A., Bansal S., Hider R., Mather S.J. (1999). Comparison of the stability of technetium-labeled peptides to challenge with cysteine. Bioconjug Chem.
15 Alberto R. (2003). [Tc(CO)(3)](+) chemistry: a promising new concept for SPET? For. Eur J Nucl Med Mol Imaging.
16 Alberto R., Ortner K., Wheatley N., Schibli R., Schubiger A.P. (2001). Synthesis and properties of boranocarbonate: a convenient in situ CO source for the aqueous preparation of [(99m)Tc(OH(2))3(CO)3]+. J Am Chem Soc.